# Anti-vascular cell adhesion molecule antibody M/K-2.7 and anti-P-selectin antibody RB40.34 conjugated microparticles of iron oxide

Chemical name: | Anti-vascular cell adhesion molecule antibody M/K-2.7 and anti-P-selectin antibody RB40.34 conjugated microparticles of iron oxide
Abbreviated name: | VCAM-MPIO-P-selectin
Synonym: | M/K-2.7-MPIO-RB40.34
Agent Category: | Antibody
Target: | Vascular cell adhesion molecule-1 (VCAM-1) and P-selectin
Target Category: | Antibody-antigen binding
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal/contrast: | Iron oxide
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=54648638), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=46249772) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=7412) for more information about VCAM-1. Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=200553), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=6031196) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=6403) for more information about P-selectin.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VCAM-1+MPIO+Selectin)]

Magnetic resonance imaging (MRI) maps information about tissues spatially and functionally. Protons (hydrogen nuclei) are widely used to create images because of their abundance in water molecules, which comprise >80% of most soft tissues. The contrast of proton MRI images depends mainly on the nuclear density (proton spins), the relaxation times of the nuclear magnetization (T_1_, longitudinal; T_2_, transverse), the magnetic environment of the tissues, and the blood flow to the tissues. However, insufficient contrast between normal and diseased tissues requires the use of contrast agents. Most contrast agents affect the T_1_ and T_2_ relaxation times of the surrounding nuclei, mainly the protons of water. T_2_* is the spin–spin relaxation time composed of variations from molecular interactions and intrinsic magnetic heterogeneities of tissues in the magnetic field (1). Cross-linked iron oxide (CLIO) nanoparticles and other iron oxide formulations affect T_2_ primarily and lead to decreased signals. On the other hand, paramagnetic T_1_ agents such as gadolinium (Gd^3+^) and manganese (Mn^2+^) accelerate T_1_ relaxation and lead to brighter contrast images.

Endothelial cells are important cells in inflammatory responses (2, 3). Bacterial lipopolysaccharide (LPS), virus, inflammation, and tissue injury increase tumor necrosis factor α (TNFα), interleukin-1 (IL-1), and other cytokine and chemokine secretion. Emigration of leukocytes from blood is dependent on their ability to roll along endothelial cell surfaces and subsequently adhere to endothelial cell surfaces. Inflammatory mediators and cytokines induce chemokine secretion from endothelial cells and other vascular cells and increase their expression of cell-surface adhesion molecules, such as intracellular adhesion molecule-1, vascular cell adhesion molecule-1 (VCAM-1), integrins, and selectins. Chemokines are chemotactic toward leukocytes and toward sites of inflammation and tissue injury. The movements of leukocytes through endothelial junctions into the extravascular space are highly orchestrated through various interactions with different adhesion molecules on endothelial cells (4).

P-selectin is found on the cell surface of endothelial cells and platelets (3, 5). It binds to glycoproteins on the cell surface of leukocytes. P-selectin and other selectins are involved in rolling and arresting leukocytes on the endothelium. VCAM-1 is found in very low levels on the cell surface of resting endothelial cells and other vascular cells, such as smooth muscle cells and fibroblasts (6-10). VCAM-1 binds to its counterligand, very late antigen-4 (VLA-4) integrin, on the cell surface of leukocytes. IL-1 and TNFα increase expression of VCAM-1, P-selectin, and other cell adhesion molecules on the vascular endothelial cells, which leads to leukocyte adhesion to the activated endothelium. Furthermore, VCAM-1 expression was also induced by oxidized low-density lipoproteins under atherogenic conditions (11). Overexpression of VCAM-1 by atherosclerotic lesions plays an important role in their progression to vulnerable plaques, which may erode and rupture. Microparticles of iron oxide (MPIOs) are composed of iron particles with diameters of ~4.5 µm. MPIO targeted with anti-VCAM-1 monoclonal antibody (mAb) M/K-2.7 and anti-P-selectin mAb RB40.34 (VCAM-MPIO-P-selectin) is being developed as a non-invasive, dual-targeted agent for VCAM-1 and P-selectin expression in vascular endothelial cells during different stages of inflammation in atherosclerosis (12).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VCAM-1+MPIO+Selectin+synthesis)]

The synthesis of VCAM-MPIO-P-selectin was described by McAteer et al. (12). The p-toluenesulphonyl-MPIOs were commercially available (Invitrogen). M/K-2.7 and RB40.34 mAbs (2.5 µg of each/10^7^ MPIO) were incubated with the activated MPIO at 37°C for 20 h. Single-targeted VCAM-MPIO or P-selectin-MPIO and IgG control MPIO (IgG-MPIO) were prepared in the same way with 5 µg of each mAb. MPIOs were washed and incubated with 0.1% BSA at 37°C for 4 h to block the remaining activated sites.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VCAM-1+MPIO+Selectin+in+vitro)]

McAteer et al. (12) performed in vitro cell-binding assays with VCAM-MPIO using mouse sEND-1 endothelial cells. Using light microscopy, VCAM-MPIO bound to only TNF-activated sEND-1 cells (R_2_ = 0.94, P = 0.03) in a dose-dependent manner, whereas IgG-MPIO did not. A corresponding decrease in MRI signal intensity of MPIO was observed MRI images at 11.7 T (R_2_ = 0.98, P = 0.01), indicating the presence of VCAM-MPIO on the cell surface. VCAM-MPIO binding was blocked by pre-incubation with soluble VCAM-1 and not with ICAM-1. Unconjugated MPIO were phagocytosed by mouse peritoneal macrophages and not by sEND-1 cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VCAM-1+MPIO+Selectin+rodentia)]

VCAM-MPIO-P-selectin (6 × 10^7^ MPIO, 30 mg iron/kg) was administered in apolipoprotein E^-/-^ mice (n = 6) (12). Using light microscopy, the number of dual-targeted MPIOs that bound to endothelium overlying aortic root atherosclerosis was 5.9-fold more than P-selectin-MPIOs (16.1 ± 2.7 per section) (n = 4) (P < 0.05) and 4.5-fold more than VCAM-MPIOs (12.9 ± 4.2) (n = 7) (P < 0.01). The number of IgG_1_-MPIOs that bound was 1.7 ± 4.2. VCAM-MPIO-P-selectin was injected intravenously in apolipoprotein E^-/-^ mice via the jugular vein (n = 4). The number of VCAM-MPIO-P-selectin that bound aortic root endothelium was quantifiable with ex vivo MRI (2.5-fold increase versus IgG_1_-MPIO (14 ± 4.2 versus 4 ± 1.8); P < 0.01). The MPIOs were well tolerated in apolipoprotein E^-/-^ mice, and histological examination showed that the lungs had high accumulation at 30 min after injection with redistribution to the spleen and liver at 24 h. No blocking experiments were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VCAM-1+MPIO+Selectin+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VCAM-1+MPIO+Selectin+(primate%20not%20human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VCAM-1+MPIO+Selectin+human)]

No publication is currently available.

## References

1 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
2 Cybulsky M.I., Gimbrone M.A. (1991). Endothelial expression of a mononuclear leukocyte adhesion molecule during atherogenesis. Science.
3 Lowe J.B. (2002). Glycosylation in the control of selectin counter-receptor structure and function. Immunol Rev.
4 Vanderslice P., Woodside D.G. (2006). Integrin antagonists as therapeutics for inflammatory diseases. Expert Opin Investig Drugs.
5 Chen M., Geng J.G. (2006). and P-selectin mediates adhesion of leukocytes, platelets, and cancer cells in inflammation, thrombosis, and cancer growth and metastasis. Arch Immunol Ther Exp (Warsz).
6 Bochner B.S., Luscinskas F.W., Gimbrone M.A., Newman W., Sterbinsky S.A., Derse-Anthony C.P., Klunk D., Schleimer R.P. (1991). Adhesion of human basophils, eosinophils, and neutrophils to interleukin 1-activated human vascular endothelial cells: contributions of endothelial cell adhesion molecules. J Exp Med.
7 Kume N., Cybulsky M.I., Gimbrone M.A. (1992). Lysophosphatidylcholine, a component of atherogenic lipoproteins, induces mononuclear leukocyte adhesion molecules in cultured human and rabbit arterial endothelial cells. J Clin Invest.
8 Leung K.H. (1999). Release of soluble ICAM-1 from human lung fibroblasts, aortic smooth muscle cells, dermal microvascular endothelial cells, bronchial epithelial cells, and keratinocytes. Biochem Biophys Res Commun.
9 Luscinskas F.W., Cybulsky M.I., Kiely J.M., Peckins C.S., Davis V.M., Gimbrone M.A. (1991). Cytokine-activated human endothelial monolayers support enhanced neutrophil transmigration via a mechanism involving both endothelial-leukocyte adhesion molecule-1 and intercellular adhesion molecule-1. J Immunol.
10 Nagel T., Resnick N., Atkinson W.J., Dewey C.F., Gimbrone M.A. (1994). Shear stress selectively upregulates intercellular adhesion molecule-1 expression in cultured human vascular endothelial cells. J Clin Invest.
11 Aikawa M., Libby P. (2004). The vulnerable atherosclerotic plaque: pathogenesis and therapeutic approach. Cardiovasc Pathol.
12 McAteer M.A., Schneider J.E., Ali Z.A., Warrick N., Bursill C.A., von zur Muhlen C., Greaves D.R., Neubauer S., Channon K.M., Choudhury R.P. (2008). Magnetic resonance imaging of endothelial adhesion molecules in mouse atherosclerosis using dual-targeted microparticles of iron oxide. Arterioscler Thromb Vasc Biol.